# 5-Methyl-8-(4-[^11^C]methyl-piperazin-1-yl)-4-oxo-4H-chromene-2-carboxylic acid (4-morpholin-4-yl-phenyl)-amide

Chemical name: | 5-Methyl-8-(4-[^11^C]methyl-piperazin-1-yl)-4-oxo-4H-chromene-2-carboxylic acid (4-morpholin-4-yl-phenyl)-amide
Abbreviated name: | [^11^C]AZ10419369
Synonym:
Agent category: | Compound
Target: | 5-HT_1B_ serotonin receptors
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[P ubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369)]

5-Hydroxytryptamine (5-HT), commonly known as serotonin, has diverse physiological roles as a neurotransmitter in the central nervous system (1). 5-HT is involved in regulation and modulation of sleep, affective and personality behaviors, and pain. It also is a regulator of smooth muscle function and platelet aggregation. The brain cortical 5-HT system has been implicated in several neuropsychiatric disorders, including major depression, anxiety, schizophrenia, and obsessive-compulsive disorder (2, 3). The effects of 5-HT are mediated by as many as seven classes of receptor populations (5-HT_1_ to 5-HT_7_), many of which include several subtypes (4). There are five receptor subtypes within the G-protein–coupled 5-HT_1_ receptor family: 5-HT_1A_, 5-HT_1B_, 5-HT_1D_, 5-HT_1E_, and 5-HT_1F_.

5-HT_1B_ Receptors are abundantly present in the pallidum, substantia nigra, ventral striatum, and visual cortex. 5-HT_1B_ Receptors are implicated in anxiety, depression, aggressive behavior, and substance abuse disorders (5-9), and these receptors play an important role in modulation of synaptic release of 5-HT (10). Thus, there is a need for selective ligands to investigate the pharmacological role of 5-HT_1B_ receptors with positron emission tomography (PET) imaging. 5-Methyl-8-(4-methyl-piperazin-1-yl)-4-oxo-4H-chromene-2-carboxylic acid (4-morpholin-4-yl-phenyl)-amide (AZ10419369) was reported to be a potent ligand of 5-HT_1B_ receptors (inhibition constant (K_i_) = 0.8 nM) (11). This led to the development of 5-methyl-8-(4-[^11^C]methyl-piperazin-1-yl)-4-oxo-4H-chromene-2-carboxylic acid (4-morpholin-4-yl-phenyl)-amide ([^11^C]AZ10419369) as a useful tool for in vivo PET imaging of the 5-HT_1B_ receptor (11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20synthesis)]

The radiosynthesis of [^11^C]AZ10419369, reported by Pierson et al. (11), involved standard ^11^C-N-methylation of the corresponding desmethyl precursor 8-(1-piperazinyl)-5-methylchrom-2-en-4-one-2-(4-morpholinophenyl)carboxamide with [^11^C]CH_3_OTf in acetone in the presence of NaOH. The reported overall radiochemical yield of the radiosynthesis was ~70% at the end of synthesis, the specific radioactivity was >133 TBq/mmol (>3,600 Ci/mmol), and the radiochemical purity was >99%. The total synthesis time was 30 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20in%20vitro)]

In vitro autoradiography studies of macaque brain slices indicated that the highest binding of [^3^H]AZ10419369 occurred in the primary visual cortex, substantia nigra, ventral striatum, and pallidum, and that the lowest binding occurred in the cerebellum, consistent with 5-HT_1B_ receptor distribution (11). The 5-HT_1B/1D_ antagonist GR 127935 (10 μM) markedly inhibited the binding in primary visual cortex. Maier et al. (12) reported a K_d_ value of 0.37 nM and a maximum binding (B_max_) of 8.76 pmol/mg protein using [^3^H]AZ10419369 binding to human 5-HT_1B_ receptor In transfected CHO cell membranes. Cross reactivity with other 5-HT subtypes was not determined.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20rodentia)]

No publication is currently available.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20nonhuman%20primate)]

PET imaging was used to study radioactivity accumulation in two macaque brains after intravenous injection of 50 MBq (1.35 mCi) [^11^C]AZ10419369 (11). Various brain regions exhibited rapid accumulation in 3–13 min with gradual decreases thereafter. The total brain accumulation was 3–4% injected dose (ID)/g at 7.5 min (peak). [^11^C]AZ10419369 PET images (up to 90 min after injection) displayed the maximum radioactivity concentrations at 40 min with tissue/cerebellum ratios that followed a rank order: the occipital cortex (4.2), striatopallidal complex (4.1), thalamus (2.6), frontal cortex (2.6), and cerebellum (1.0). Pretreatment with the 5-HT_1B_ selective antagonist AR-A000002 (1–2 mg/kg) 30 min prior to injection of [^11^C]AZ10419369 markedly reduced the radioactivity in the occipital cortex by 50–70% with little effect in the cerebellum. After injection of [^11^C]AZ10419369, 95% and 74% of the total plasma radioactivity was intact at 4 and 30 min, respectively. Only hydrophilic metabolites were detected.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=AZ10419369%20and%20human)]

PET imaging was used to study radioactivity accumulation in two human brains after intravenous injection of 302 MBq (8.16 mCi) [^11^C]AZ10419369 (11). Various brain regions exhibited rapid accumulation in 3–13 min with slow decreases thereafter. The total brain accumulation was 3–4% ID/g at 7.5 min (peak). [^11^C]AZ10419369 PET images (up to 90 min after injection) displayed maximum radioactivity concentrations at 30 min with tissue/cerebellum ratios that followed a rank order: the globus pallidus (3.2), ventral striatum (2.7), occipital cortex (2.2), caudate nucleus (1.9), thalamus (1.3), and cerebellum (1.0). This rank order is consistent with that seen in macaques in vitro and in vivo. After injection of [^11^C]AZ10419369, >97% of the total plasma radioactivity was intact at 20 min.

## References

1 Lucki I. (1998). The spectrum of behaviors influenced by serotonin. Biol Psychiatry.
2 Fletcher A., Cliffe I.A., Dourish C.T. (1993). Silent 5-HT1A receptor antagonists: utility as research tools and therapeutic agents. Trends Pharmacol Sci.
3 Hoyer D., Clarke D.E., Fozard J.R., Hartig P.R., Martin G.R., Mylecharane E.J., Saxena P.R., Humphrey P.P. (1994). International Union of Pharmacology classification of receptors for 5-hydroxytryptamine (Serotonin). Pharmacol Rev.
4 Lanfumey L., Hamon M. (2004). 5-HT1 receptors. Curr Drug Targets CNS Neurol Disord.
5 Cowen P.J. (2000). Psychopharmacology of 5-HT(1A) receptors. Nucl Med Biol.
6 Massot O., Rousselle J.C., Grimaldi B., Cloez-Tayarani I., Fillion M.P., Plantefol M., Bonnin A., Prudhomme N., Fillion G. (1998). Molecular, cellular and physiological characteristics of 5-HT-moduline, a novel endogenous modulator of 5-HT1B receptor subtype. Ann N Y Acad Sci.
7 Meneses A. (1999). 5-HT system and cognition. Neurosci Biobehav Rev.
8 Olivier, B., Serotonergic mechanisms in aggression. Novartis Found Symp, 2005268: p. 171-83; discussion 183-9, 242-53.
9 Barnes N.M., Sharp T. (1999). A review of central 5-HT receptors and their function. Neuropharmacology.
10 Engel G., Gothert M., Hoyer D., Schlicker E., Hillenbrand K. (1986). Identity of inhibitory presynaptic 5-hydroxytryptamine (5-HT) autoreceptors in the rat brain cortex with 5-HT1B binding sites. Naunyn Schmiedebergs Arch Pharmacol.
11 Pierson M.E., Andersson J., Nyberg S., McCarthy D.J., Finnema S.J., Varnas K., Takano A., Karlsson P., Gulyas B., Medd A.M., Lee C.M., Powell M.E., Heys J.R., Potts W., Seneca N., Mrzljak L., Farde L., Halldin C. (2008). [11C]AZ10419369: a selective 5-HT1B receptor radioligand suitable for positron emission tomography (PET). Characterization in the primate brain. Neuroimage.
12 Maier, D.L., C. Sobotka-Briner, M. Ding, M.E. Powell, Q. Jiang, G. Hill, J.R. Heys, C.S. Elmore, M.E. Pierson, and L. Mrzljak, [N-methyl-3H3]AZ10419369 binding to the 5-HT1B receptor: in vitro characterization and in vivo receptor occupancy. J Pharmacol Exp Ther, 2009